# 2-(6-[^11^C]Methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-7-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-9H-fluoren-9-one

Chemical name: | 2-(6-[^11^C]Methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-7-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-9H-fluoren-9-one
Abbreviated name: | [^11^C]A-752274
Synonym:
Agent Category: | Compound
Target: | α7-Nicotinic acetylcholine receptor (α7-nAChR)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the structure of [^11^C]A-752274 for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Function%20of%20nicotinic%20acetylcholine%20receptors&cmd=DetailsSearch)]

The nicotinic acetylcholine receptors (nAChR) are pentameric ligand-gated cation channels that are found primarily in the central nervous system of mammals and are composed of α and β subunits arranged in various homomeric or heteromeric stoichiometric arrangements (for details, see dos Santos Coura and Granon (1)). The nAChRs have a high affinity for both nicotine and acetylcholine; binding of a ligand to the receptor facilitates the passage of cations into the cell, which alters the polarity of the cell membrane and activates signal transduction pathways that culminate in a cellular response (2). These receptors are believed to be involved in a variety of physiological processes, such as cognitive functions (1), neuroprotection in Parkinson’s disease (3), Alzheimer’s disease (AD) (4), and the progression of certain cancers (5). The heteromeric α4β2 and the homomeric α7 are the most commonly expressed nAChRs in the brain, and the β2 subunit is a component of most heteromeric nicotinic receptors in the central nervous system. There is much evidence that α4β2-nAChR is involved in normal cognitive functions in animals; it is also implicated in addiction (e.g., smoking) and in the cognitive impairments observed with AD, attention deficit hyperactivity disorder, and schizophrenia (6). α7-nAChR participates in cognitive processes and has a reduced expression in the human schizophrenic brain, and there are indications that it has a therapeutic role in the treatment of AD (7).

Although some radiolabeled compounds can be used with positron emission tomography (PET) for the imaging of α4β2-nAChR in the human brain (8), no suitable tracer(s) are available for the noninvasive investigation of α7-nAChR in humans (7). In an effort to develop new ligands for α7-nAChR, two compounds, 2-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-7-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-9H-fluoren-9-one (A-752274) and 5-(6-(5-methylhexahydropyrrolo[3,4-c]pyrrol-2(1H)-yl)pyridazin-3-yl)-1H-indole (A-833834) were synthesized and labeled with ^11^C ([^11^C]A-752274 and [^11^C]A-833834, respectively) (7). The biodistribution of both tracers was investigated in the mouse brain, and [^11^C]A-752274 was also evaluated for PET imaging of the brain of a baboon. This chapter presents results obtained with [^11^C]A-752274. The biodistribution characteristics of [^11^C]A-833834 are discussed in a separate chapter in MICAD (www.micad.nih.gov) (9).

### Related Resource Links

nAChR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?cmd=Search&term=nAChR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log$=booksrch&bname=micad)

Human α7-nAChR (http://www.ncbi.nlm.nih.gov/gene/1139) in Gene Database; Gene ID: 1139

α7-nAChR in Online Mendelian Inheritance in Man (OMIM (http://omim.org/entry/118511)) Database

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=nAChR) related to nAChRs

nAChRs as drug targets [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?itool=pubmed_Abstract&DbFrom=pubmed&Cmd=Link&LinkName=pubmed_pubmed&IdsFromResult=21631405&retmode=ref)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-752274%20synthesis&cmd=DetailsSearch)]

The synthesis of A-752274 and its labeling with ^11^C has been described by Horti et al. (7). The total time required for the synthesis of [^11^C]A-752274 was 39 min. The identity of [^11^C]A-752274 was confirmed with coinjection of the corresponding non-radiolabeled compound for analysis on a high-performance liquid chromatography (HPLC) column. The radiochemical yield of [^11^C]A-752274 with respect to [^11^C]methyl triflate (used to label the receptor ligand) was 12 ± 4%. The specific activity of [^11^C]A-752274 was 332 ± 51 GBq/μmol (12.3 ± 1.89 Ci/μmol), with a radiochemical purity of 99% as determined with HPLC analysis at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-752274%20in%20vitro%20studies&cmd=DetailsSearch)]

The binding affinity of A-752274 for α7-nAChR was determined in a displacement assay that used rat brain membrane preparations (without the cerebellum) with [^3^H]-(S,S)-2,2-dimethyl-5-(6-phenyl-pyridazin-3-yl)-5-aza-2-azonia-bicyclo[2.2.1]heptane iodide as the radioligand (7). The K_i_ of A-752274 was reported to be 0.092 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-752274%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]A-752274 was investigated in the brain tissue of normal CD1 mice (7). The animals (n = 3 animals/time point) were injected with ~100 μCi [^11^C]A-752274 through the lateral tail vein, and the rodents were euthanized at preselected time points (maximum of 90 min postinjection (p.i.)) to remove their brains and determine the amount of radioactivity present in the various regions of the organ. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). Maximum accumulation of label was observed in the thalamus (0.9% ID/g; this area of the brain has a high level of α7-nAChR), followed by the superior colliculus (0.8% ID/g) and the hippocampus (0.6% ID/g). The thalamus/cerebellum, superior colliculus/cerebellum, and hippocampus/cerebellum uptake ratios continued to increase with time and did not peak even at the end of the study. At 90 min p.i., the uptake ratios were 2.1, 1.8, and 1.4, respectively. A very high level of label was observed in the adrenal glands (~20% ID/g) because these glands have a very high expression of α7-nAChR compared with the other regions of the brain.

To establish the receptor-binding specificity of [^11^C]A-752274, the mice (n = 3 animals/time point) were injected with a mixture of 100 μCi tracer and 0.1 mg/kg body weight non-radioactive A-752274 as described above (7). The rodents were euthanized at 90 min p.i., and the amount of radioactivity in the different regions of the brain was determined. Compared with the control mice that received only [^11^C]A-752274, the amount of radioactivity in the thalamus of the blocked animals was reduced by ~50% (P < 0.05). Almost no difference was observed in the amount of tracer present in the cerebellum of the control and the blocked rodents (P > 0.05). These observations indicated that [^11^C]A-752274 had a high binding specificity for α7-nAChR.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-752274%20non-primate%20mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-752274%20Non-Human%20Primates&cmd=DetailsSearch)]

In general, the distribution of α7-nAChR in the non-human primate brain is believed to be similar to that in the mouse brain (hippocampus ≈ thalamus > cortical regions and basal ganglia > cerebellum), but a detailed map of the receptor in the non-human primate brain is not available (7). Because [^11^C]A-752274 showed a high binding specificity for α7-nAChR in the mouse studies, a single baboon was injected with the radiotracer to acquire PET images of the non-human primate brain(details of this study were not reported). PET images acquired at 90 min p.i. showed that the amount of tracer in the baboon brain was insufficient for accurate data analysis. HPLC analysis of the baboon plasma at 90 min p.i. showed the presence of several metabolites of [^11^C]A-752274, and only 7% of the parent radiolabeled compound was determined to be intact at this time point.

From these studies on mice and the baboon, the investigators concluded that it is necessary to develop more compounds that are based on A-752274 to investigate the biological characteristics of α7-nAChR (7). In addition, these compounds should have a strong affinity for α7-nAChR, and they should exhibit high permeability through the blood–brain barrier (7).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-752274%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were supported by National Institutes of Health grants DA020777 and MH079017.

## References

1 dos Santos Coura R., Granon S. (2012). Prefrontal neuromodulation by nicotinic receptors for cognitive processes. Psychopharmacology (Berl).
2 Albuquerque E.X., Pereira E.F., Alkondon M., Rogers S.W. (2009). Mammalian nicotinic acetylcholine receptors: from structure to function. Physiol Rev.
3 Kawamata J., Suzuki S., Shimohama S. (2012). alpha7 nicotinic acetylcholine receptor mediated neuroprotection in Parkinson's disease. Curr Drug Targets.
4 Hernandez C.M., Dineley K.T. (2012). alpha7 nicotinic acetylcholine receptors in Alzheimer's disease: neuroprotective, neurotrophic or both?. Curr Drug Targets.
5 Schuller H.M. (2012). Regulatory role of the alpha7nAChR in cancer. Curr Drug Targets.
6 Radek R.J., Kohlhaas K.L., Rueter L.E., Mohler E.G. (2010). Treating the cognitive deficits of schizophrenia with alpha4beta2 neuronal nicotinic receptor agonists. Curr Pharm Des.
7 Horti A.G., Ravert H.T., Gao Y., Holt D.P., Bunnelle W.H., Schrimpf M.R., Li T., Ji J., Valentine H., Scheffel U., Kuwabara H., Wong D.F., Dannals R.F. (2013). Synthesis and evaluation of new radioligands [(11)C]A-833834 and [(11)C]A-752274 for positron-emission tomography of alpha7-nicotinic acetylcholine receptors. Nucl Med Biol.
8 Horti A.G., Wong D.F. (2009). Clinical Perspective and Recent Development of PET Radioligands for Imaging Cerebral Nicotinic Acetylcholine Receptors. PET Clin.
9 Chopra, A., 5-(6-(5-[11C]methylhexahydropyrrolo[3,4-c]pyrrol-2(1H)-yl)pyridazin-3-yl)-1H-indole. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.